# [^11^C]2-2-(Dimethylaminomethyl)phenylthio)-5-fluorophenylamine

Chemical name: | [^11^C]2-(2-(Dimethylaminomethyl)phenylthio)-5-fluorophenylamine
Abbreviated name: | [^11^C]AFA
Synonym:
Agent Category: | Compound
Target: | Serotonin transporter (SERT)
Target Category: | Ligand binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%5BAll%20Fields%5D%20AND%20AFA%5BAll%20Fields%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?CMD=search&DB=pubmed]

A number of neuropsychiatric disorders, including major depression, schizophrenia, Alzheimer’s disease, and Parkinson’s disease (1-3), involve a dysfunction of the brain’s serotonin system. The serotonergic neurons – present in large areas of the brain, including the hypothalamus, thalamus, and cerebral cortex – bear a protein called ‘serotonin transporter’ (SERT) (4).

The SERT is a specific marker for the number and integrity of presynaptic terminals of serotonin-producing neurons. It regulates neurotransmission by removing released serotonin from the extracellular space back into the presynaptic neuron. Commonly prescribed antidepressants are selective serotonin reuptake inhibitors, and their effects are obtained through interaction with the SERT (5).

A variety of radioligands for positron emission tomography (PET) have been evaluated for imaging the SERT. The most recent include [^11^C]DASB, [^11^C]AFM, [^11^C]AFE, [^11^C]ADAM, [^11^C]HOMADAM. 2-(2-(Dimethylaminomethyl)phenylthio)-5-fluorophenylamine (AFA), a novel PET radioligand, can be labeled with either ^11^C or ^18^F. In vitro, it has shown rapid brain uptake kinetics as well as a high affinity for SERT, with lower affinities for the norepinephrine transporter (NET) and dopamine transporter (DAT).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20synthesis)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fluoroflumazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D]

[^11^C]AFA can be prepared from its monomethylamino precursor, (5-fluoro-2[2-(methylaminomethylphenylthio)]phenylamine, by reaction with [^11^C]methyl iodide ([^11^C]MeI). The precursor is obtained following a protocol described in details by Huang et al. (6). The radiolabeling method involves dissolving the precursor in N, N-dimethylformamide (DMF), and bubbling [^11^C]MeI through the solution at -10 °C. After the maximum radioactivity is obtained, the solution is heated at 85 °C for 5 min in a water bath. After a multi-step purification (by HPLC), dilution with water (100mL) and passage through a Waters C_18_ Sep-Pak, the solution is then eluted in ethanol. The eluted [^11^C]AFA is mixed with sterile saline (0.9% NaCl), filtered through a 0.22 μm membrane filter, and collected in a sterile vial.

The chemical and radiochemical purity of [^11^C]AFA produced by this method is >95%, and the radiochemical yield is 43 ± 20% (decay-corrected, based on [^11^C]MeI; n = 10) (6). The specific activity of the radiotracer at the end of the synthesis is 2.13 ± 1.37 Ci/mmol (7.88 ± 5.07 GBq/mmol). The total synthesis time is about 35 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20in%20vitro)]

Comparative in vitro studies using cloned human monoamine transporters and the radioligands [^3^H]paroxetine, [^3^H]nisoxetine, and [^3^H]GBR2935 were performed by Huang et al. (6) to assess the affinity of [^11^C]AFA for the SERT, NET and DAT. Results showed a high affinity for the SERT (K_i_ = 1.46 ± 0.15 nM) and much lower affinities for the NET (K_i_ = 141.7 ± 47.4 nM) and DAT (K_i_ > 10^4^ nM). [^11^C]AFA showed virtually no affinity for benzodiazepine, serotonin, and dopamine receptors such as 5-HT_1A_, 5-HT_2c_, 5-HT_3_, 5-HT_6_, 5-HT_7_ and D_1_ through D_5_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20rodentia%5BMeSH%5D)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%22rodentia%22]

Biodistribution studies were performed ex-vivo on Sprague-Dawley rats by Huang et al. The experimental procedure involved injecting 3.7 MBq (100 μCi) of [^11^C]AFA into each animal (via the tail vein) and measuring the uptake of the radiotracer at 10, 30, 60, and 90 min post injection, after sacrifice.

Results showed rapid uptake of [^11^C]AFA into the brain, with accumulation in regions rich in SERTs. The highest levels were found in the thalamus and hypothalamus, followed by the frontal cortex, striatum, and hippocampus. The reported hypothalamus/cerebellum activity ratios were 5.32 ± 0.49 and 6.38 ± 1.32, respectively, at 60 and 120 min post injection.

When pretreated with either cold AFA (2 mg/kg of tissue) or citalopram (a selective serotonin reuptake inhibitor), about 50 to 66% of the specific binding was found to be displaced at 45 min after injection of the tracer. In contrast, pretreatment with nisoxetine (a selective norepinephrine reuptake inhibitor) did not lead to a significant change with respect to [^11^C]AFA specific binding in SERT-rich regions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20%28pig%20OR%20sheep%20OR%20rabbit%20OR%20dog%29)http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HOMADAM%20AND%20%28dog%20OR%20sheep%20OR%20pig%29]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20%28primate%20NOT%20human%29)]

Huang et al. (6) performed PET brain imaging studies of baboons for time periods ranging from 0 to 120 min after administration of [^11^C]AFA (injected dose ~185 MBq (5 mCi); specific activity at time of injection, 1854 ± 1106 Ci/mmol (68.6 GBq/μmol). The highest tracer levels of the tracer were found in regions of high SERT density (e.g., thalamus, midbrain and striatum), and the lowest levels were found in the cerebellum. [^11^C]AFA exhibited rapid uptake kinetics, with peak activity levels between 15 and 40 min post-injection.

When the baboons were pretreated with 4.8 ± 0.5 mCi of citalopram (a selective serotonin reuptake inhibitor) 20 min before injection of [^11^C]AFA, the radiotracer uptakes in the midbrain, thalamus, striatum, hippocampus, and cortex were reduced to the level in the cerebellum, showing significant reduction in the specific binding of [^11^C]AFA in all SERT-containing brain regions. A kinetic analysis done by the authors of the study (6) showed that the regional equilibrium specific-to-nonspecific partition coefficients of [^11^C]AFA were similar to those obtained for the imaging agent [^11^C]McN5652, but lower than those obtained for [^11^C]DASB (e.g., midbrain partition coefficients were 0.95 ± 0.07 and 1.68 ± 0.21 for [^11^C]AFA and [^11^C]DASB respectively).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%29AFA%20AND%20%28human%20NOT%20baboon%29)]

No publication is currently available.

## References

1 Owens MJ Nemeroff CB The serotonin transporter and depression Depress Anxiety 1998 8Suppl 15 12 9809208
2 Palmer AM, Francis PT, Benton JS, Sims NR, Mann DM, Neary D, Snowden JS, Bowen DM. (1987). Presynaptic serotonergic dysfunction in patients with Alzheimer's disease. J Neurochem.
3 Roth BL, Xia Z. (2004). Molecular and cellular mechanisms for the polarized sorting of serotonin receptors: relevance for genesis and treatment of psychosis. Crit Rev Neurobiol.
4 Laakso A, Hietala J. (2000). PET studies of brain monoamine transporters. Curr Pharm Des.
5 White KJ, Walline CC, Barker EL. (2005). Serotonin transporters: implications for antidepressant drug development. Aaps J.
6 Huang Y, Narendran R, Bae SA, Erritzoe D, Guo N, Zhu Z, Hwang DR, Laruelle M. (2004). A PET imaging agent with fast kinetics: synthesis and in vivo evaluation of the serotonin transporter ligand [11C]2-[2-dimethylaminomethylphenylthio)]-5-fluorophenylamine ([11C]AFA). Nucl Med Biol.